# Gadolinium-HU-308-incorporated micelles

Chemical name: | Gadolinium-HU-308-incorporated micelles
Abbreviated name: | CB2R-Targeted micelles
Synonym:
Agent category: | Compound
Target: | Cannabinoid receptor 2 (CNR2 or CB2)
Target category: | Receptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure (HU-308) for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles)]

There are two subtypes of cannabinoid receptors in mammalian tissues: CB1 and CB2 (1, 2). CB1 is expressed abundantly in neuronal terminals in the central nervous system (CNS) and in some peripheral tissues to inhibit neurotransmitter release. CB1 is found predominately in the striatum, hippocampus, substantia nigra, globus pallidus, and cerebellum. CB2 is present mainly on immune cells in the blood and peripheral tissues (the spleen) to modulate cytokine release (3). However, CB2 has been found in the CNS tissues (neurons and glial cells) at very low levels (4). Both receptor subtypes are coupled through G_i/o_ proteins to inhibit adenylate cyclase and to modulate potassium and calcium channels. CB1 has been shown to be involved in analgesia, regulation of food intake, and control of movement in normal subjects (3). Alteration of CB1 function has been implicated in a number of human diseases such as depression, schizophrenia, and obesity (5-7). Upregulation of CB2 in the brain is associated with neuroinflammation in disorders such as Alzheimer’s disease, multiple sclerosis, encephalitis, and Down’s syndrome (8). CB2 is also involved in inflammation associated with pain, osteoporosis, cancer, and liver diseases (9).

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (10, 11). Gd-Diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous magnetic resonance imaging (MRI) contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancerous tissues. Various macromolecular Gd complexes have demonstrated superior contrast enhancement for MRI of the vasculature and carcinomas (12-14); however, these Gd complexes cannot proceed into further clinical development because of high tissue accumulation and slow excretion of toxic Gd ions. Furthermore, they are largely nonspecific.

HU-308 is a potent selective CB2 agonist in vitro and in mice (15, 16). HU-308 and Gd-DTPA were incorporated into di-stearoyl-polyethylene glycol-phosphatidylethanolamine 2000 (DSPE-PEG2000) micelles (CB2R-targeted micelles) for MRI of vulnerable atherosclerotic plaques (17, 18).

### Related Resource Links:

- Chapters in MICAD (CB2 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=(CB2%20OR%20CB1)+AND+micad%5Bbook%5D))
- Gene information in NCBI (CB2 (http://www.ncbi.nlm.nih.gov/gene/1269))
- Articles Online Mendelian Inheritance in Man (OMIM) (CB2 (http://www.ncbi.nlm.nih.gov/omim/605051))
- Clinical trials (CB2 (http://www.clinicaltrials.gov/ct2/results?term=CB2))
- Drug information in FDA (CB2 (http://google2.fda.gov/search?q=CB2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+synthesis)]

A mixture of DSPE-PEG2000, Gd-DTPA-bisstearylamide, lissamine-rhodamine-phosphatidylethanolamine, and HU-308 in a molar ratio of 35:50:5:10 in chloroform was dried by rotary evaporation for 3 min at 40°C (18). The lipid film was subsequently hydrated for 5 min with 1 ml phosphate-buffered saline to a final lipid concentration of 10 mM and a final Gd-DTPA-bisstearylamide concentration of 5 mM. Control micelles were prepared similarly in a molar ratio of 45:5:50 without HU-308. CB2-Targeted and control micelles had diameters of 16.5 ± 1.2 nm and 19 ± 1 nm, respectively, as determined with dynamic light scattering. CB2R-Targeted micelles exhibited an r1 relaxivity value of 2.7 mM^-1^s^-1^ in phosphate-buffered saline at 9.4 T and 37°C, whereas Gd-DTPA exhibited an r1 relaxivity value of 1.8 mM^-1^s^-1^ under the same conditions.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+in+vitro)]

CB2R-Targeted micelles showed upregulation of mitogen-activated protein kinase in Chinese hamster ovary (CHO) cells transfected with CB2 but not in CHO cells without CB2 after 15 min of incubation (18). Binding studies showed that MRI contrast enhancement was only observed in CHO cells positive for CB2 with CB2R-targeted micelles and not with control micelles.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+rodentia)]

te Boekhorst et al. (18) used a 9.4-T MRI scanner to perform in vivo MRI in apolipoprotein E–deficient/endothelial nitric oxide synthase deficient (ApoE^-/-^/eNOS^-/-^) mice, which exhibit severe atherosclerosis in the abdominal area. CB2R-Targeted micelles (n = 9, 67 µmol/kg Gd), control micelles (n = 9, 67 µmol/kg Gd), and Gd-DTPA (n = 3, 300 µmol/mouse) were injected in the mice. Both CB2R-targeted and control micelles accumulated in aortic plaque within 15 min after injection as observed with MRI. After a few hours, lymph node and liver enhancement were also observed, whereas kidney, spleen and pre-vertebral muscle did not show enhancement. The normalized enhancement ratio (NER_CB2R_ versus control) for aortic plaque remained stable at 42 h and 48 h (1.95 ± 0.29, 1.90 ± 0.33, respectively) after injection with CB2R-targeted micelles, whereas NER_Control_ (1.13 ± 0.18, 1.22 ± 0.15, respectively) decreased to preinjection levels at 42 h and 48 h after injection of control micelles (P < 0.05–0.01). NER_Gd-DTPA_ peaked at 1.57 ± 0.12 at 1.5 h after injection of Gd-DTPA, returning to baseline levels at 2.5 h. NER_lymph node_ was 1.3 at 12 h after injection of CB2R-targeted micelles, and NER_liver_ was 1.5 at 24 h after injection of CB2R-targeted micelles. The Gd levels in the excised atherosclerotic aorta at 24 h after injection of targeted and control micelles were 4.38 ± 8.34 and 3.63 ± 2.50 µg/g, respectively. At 48 h, the Gd levels were 3.31 ± 1.57 and 1.61 ± 0.45 µg/g for targeted and control micelles (P < 0.05), respectively. Immunohistochemical staining showed that CB2R-targeted micelles were colocalized with macrophages in the aortic plaque. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CB2%20micelles+human)]

No publication is currently available.

## References

1 Howlett A.C., Barth F., Bonner T.I., Cabral G., Casellas P., Devane W.A., Felder C.C., Herkenham M., Mackie K., Martin B.R., Mechoulam R., Pertwee R.G. (2002). International Union of Pharmacology. XXVII. Classification of cannabinoid receptors. Pharmacol Rev.
2 Pertwee R.G. (1997). Pharmacology of cannabinoid CB1 and CB2 receptors. Pharmacol Ther.
3 Pertwee, R.G., Pharmacological actions of cannabinoids. Handb Exp Pharmacol, 2005(168): p. 1-51.
4 Onaivi E.S., Ishiguro H., Gong J.P., Patel S., Perchuk A., Meozzi P.A., Myers L., Mora Z., Tagliaferro P., Gardner E., Brusco A., Akinshola B.E., Liu Q.R., Hope B., Iwasaki S., Arinami T., Teasenfitz L., Uhl G.R. (2006). Discovery of the presence and functional expression of cannabinoid CB2 receptors in brain. Ann N Y Acad Sci.
5 Gambi F., De Berardis D., Sepede G., Quartesan R., Calcagni E., Salerno R.M., Conti C.M., Ferro F.M. (2005). Cannabinoid receptors and their relationships with neuropsychiatric disorders. Int J Immunopathol Pharmacol.
6 De Vries T.J., Schoffelmeer A.N. (2005). Cannabinoid CB1 receptors control conditioned drug seeking. Trends Pharmacol Sci.
7 Guzman M., Sanchez C. (1999). Effects of cannabinoids on energy metabolism. Life Sci.
8 Benito C., Tolon R.M., Pazos M.R., Nunez E., Castillo A.I., Romero J. (2008). Cannabinoid CB2 receptors in human brain inflammation. Br J Pharmacol.
9 Pertwee R.G. (2009). Emerging strategies for exploiting cannabinoid receptor agonists as medicines. Br J Pharmacol.
10 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
11 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
12 Schmiedl U., Ogan M., Paajanen H., Marotti M., Crooks L.E., Brito A.C., Brasch R.C. (1987). Albumin labeled with Gd-DTPA as an intravascular, blood pool-enhancing agent for MR imaging: biodistribution and imaging studies. Radiology.
13 Gossmann A., Okuhata Y., Shames D.M., Helbich T.H., Roberts T.P., Wendland M.F., Huber S., Brasch R.C. (1999). Prostate cancer tumor grade differentiation with dynamic contrast-enhanced MR imaging in the rat: comparison of macromolecular and small-molecular contrast media--preliminary experience. Radiology.
14 Preda A., van Vliet M., Krestin G.P., Brasch R.C., van Dijke C.F. (2006). Magnetic resonance macromolecular agents for monitoring tumor microvessels and angiogenesis inhibition. Invest Radiol.
15 Rajesh M., Pan H., Mukhopadhyay P., Batkai S., Osei-Hyiaman D., Hasko G., Liaudet L., Gao B., Pacher P. (2007). Cannabinoid-2 receptor agonist HU-308 protects against hepatic ischemia/reperfusion injury by attenuating oxidative stress, inflammatory response, and apoptosis. J Leukoc Biol.
16 Hanus L., Breuer A., Tchilibon S., Shiloah S., Goldenberg D., Horowitz M., Pertwee R.G., Ross R.A., Mechoulam R., Fride E. (1999). HU-308: a specific agonist for CB(2), a peripheral cannabinoid receptor. Proc Natl Acad Sci U S A.
17 te Boekhorst B.C., Bovens S.M., van de Kolk C.W., Cramer M.J., Doevendans P.A., ten Hove M., van der Weerd L., Poelmann R., Strijkers G.J., Pasterkamp G., van Echteld C.J. (2010). The time window of MRI of murine atherosclerotic plaques after administration of CB2 receptor targeted micelles: inter-scan variability and relation between plaque signal intensity increase and gadolinium content of inversion recovery prepared versus non-prepared fast spin echo. NMR Biomed.
18 te Boekhorst B.C., Bovens S.M., Rodrigues-Feo J., Sanders H.M., van de Kolk C.W., de Kroon A.I., Cramer M.J., Doevendans P.A., ten Hove M., Pasterkamp G., van Echteld C.J. (2010). Characterization and in vitro and in vivo testing of CB2-receptor- and NGAL-targeted paramagnetic micelles for molecular MRI of vulnerable atherosclerotic plaque. Mol Imaging Biol.